# Cy5.5-Asp-Gly-Glu-Ala-Gly-Lys-(Arg)_8_-OH

Chemical name: | Cy5.5-Asp-Gly-Glu-Ala-Gly-Lys-(Arg)_8_-OH
Abbreviated name: | Cy5.5-DGEAGK(R8)-OH
Synonym:
Agent category: | Peptide
Target: | Integrin α_2_β_1_
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAF77577.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_002203.3) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3673) for more information about integrin α_2_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA)]

Integrin receptors are a family of cell-surface heterodimeric glycoproteins that mediate diverse biological events (e.g., cell adhesion, migration, differentiation, proliferation, and apoptosis) involving cell–cell and cell–matrix interactions (1, 2). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. On the other hand, integrins affect tumor growth, tumor invasiveness, and metastasis (3, 4). The α_2_β_1_ integrin binds mainly to collagen type I, laminins, E-cadherin, and matrix metalloproteinase 1 (5). The α_2_β_1_ integrin is strongly expressed on tumor cells and has been implicated in tumor progression and metastasis (6, 7). In particular, prostate cancer cells and prostate cancer stem cells express high levels of α_2_β_1_ integrin (8, 9). A tetrapeptide sequence consisting of Asp-Gly-Glu-Ala (DGEA) has been identified as a recognition motif used by the type I collagen to bind to α_2_β_1_ integrin (10). DGEA was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in prostate tumor-bearing mice (11). Cy5.5-DGEA exhibited high accumulation in the α_2_β_1_-positive PC-3 human prostate tumor cells and kidneys in nude mice. Optical and positron emission tomography imaging with various DGEA peptides showed high kidney accumulation and high tumor washout rates (11-13). To induce high tumor retention, multiple Arg molecules have been added to DGEA to help cell penetration (14). A small linker (Gly-Lys-OH) was added to the C-terminal Ala of DGEA to reduce kidney accumulation (15). The Gly-Lys bond is cleaved by the kidney brush border Lys-specific carboxypeptidase before entering the proximal tubule cells for kidney clearance. Huang et al. (16) prepared Cy5.5-Asp-Gly-Glu-Ala-Gly-Lys-(Arg)_8_-OH (Cy5.5-DGEAGK(R8)-OH) for optical imaging in mice bearing α_2_β_1_-positive PC-3 prostate tumors with lower kidney accumulation and better tumor retention than Cy5.5-DGEAGK(R4)-OH and R4-DGEAGK(Cy5.5)-OH.

### Related Resource Links:

- Chapters in MICAD (DGEA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=DGEA+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_2_ integrin (http://www.ncbi.nlm.nih.gov/gene/3673), β_1_ integrin (http://www.ncbi.nlm.nih.gov/gene/3688))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_2_ integrin (http://www.ncbi.nlm.nih.gov/omim/192974), β_1_ integrin (http://www.ncbi.nlm.nih.gov/omim/135630))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+synthesis)]

DGEAGK(R8)-OH, DGEAGK(R4)-OH, and R4-DGEAGK-OH peptides were obtained using solid-phase synthesis (16). Cy5.5-N-hydroxysuccinimide (NHS) ester was used to conjugate these DGEA peptides using solid-phase synthesis. The NHS ester of Cy5.5 reacted with the N-terminal amino group of the Asp of DGEAGK(R8)-OH and DGEAGK(R4)-OH peptides to form Cy5.5-DGEAGK(R8)-OH and Cy5.5-DGEAGK(R4)-OH. The NHS ester of Cy5.5 reacted with the Ɛ-amino group on the C-terminal Lys of R4-DGEAGK to form R4-DGEAGK(Cy5.5)-OH. The measured masses of the Cy5.5-conjugates confirmed the 1:1 conjugation of Cy5.5 to the peptides. The chemical purity was >98% after high-performance liquid chromatography purification. Cy5.5 is a NIR fluorescence dye with absorbance maximum at 675 nm and emission maximum at 694 nm, with a high extinction coefficient of 250,000 M−^1^cm−^1^. 5-Carboxyfluorescein-DGEA (FAM-DGEA) and R4-FAM-DGEA peptides were similarly prepared for in vitro studies.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+and+in+vitro)]

Flow cytometry analysis showed that 99.7% of PC-3 cells, 51.4% of CWR-22 cells, and 15.6% of LNCaP cells were positive for the α_2_β_1_ receptors using FAM-DGEA (16). The fluorescence intensity of PC-3 cells was three- to five-fold higher than that of CWR-22 and LNCaP cells, which correlated well with their α_2_β_1_ expression levels. Binding of 1 µM FAM-DGEA to the three cell types was analyzed with fluorescence microscopy. PC-3 cells exhibited a higher fluorescence intensity signal than CWR-22 and LNCaP cells. The binding of FAM-DGEA to PC-3 cells was completely blocked with 20 µM DGEA. R4-FAM-DGEA exhibited approximately two-fold higher fluorescence intensity than FAM-DGEA in all three cell lines. The binding of R4-FAM-DGEA to these cells was inhibited with DGEA. Fluorescence microscopy analysis showed nuclear accumulation of R4-FAM-DGEA in PC-3 cells, whereas FAM-DGEA fluorescence was confined to the cell surface and cytosol.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+rodentia)]

Huang et al. (16) performed NIR fluorescence imaging of nude mice bearing PC-3 (high α_2_β_1_ expression) or CWR-22 (low α_2_β_1_ expression) tumors at 0.5–4 h after intravenous injection of 1.5 nmol R4-DGEAGK(Cy5.5)-OH, Cy5.5-DGEAGK(R4)-OH, or Cy5.5-DGEAGK(R8)-OH (n = 3 mice/group). The tumor accumulation of R4-DGEAGK(Cy5.5)-OH in PC-3 tumors could be clearly visualized from 0.5 h to 4 h, reaching a maximum contrast at 4 h. The kidney accumulation was only slightly higher than the PC-3 tumor accumulation. The PC-3 tumor accumulation was significantly higher than the CWR-22 tumor accumulation (P < 0.05). The PC-3 tumor accumulation of Cy5.5-DGEAGK(R4)-OH reached a maximum at 1 h and then declined. However, the kidney accumulation was similar to the PC-3 tumor accumulation. The PC-3 tumor accumulation was significantly higher than the CWR-22 tumor accumulation (P < 0.05). The PC-3 tumor accumulation of Cy5.5-DGEAGK(R8)-OH reached a maximum at 0.5 h and then declined. However, the kidney accumulation was lower than the PC-3 tumor accumulation at each time point studied. The PC-3 tumor accumulation was significantly higher than the CWR-22 tumor accumulation (P < 0.05). Cy5.5-DGEAGK(R8)-OH exhibited higher PC-3 tumor accumulation than R4-DGEAGK(Cy5.5)-OH and Cy5.5-DGEAGK(R4)-OH. Immunohistochemistry staining of PC-3 tumor sections showed accumulation of Cy5.5-DGEAGK(R8)-OH inside the PC-3 tumor cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+human)]

No publication is currently available.

## NIH Support

P30 CA014089

## References

1 Hynes R.O. (2009). The extracellular matrix: not just pretty fibrils. Science.
2 Barczyk M., Carracedo S., Gullberg D. (2010). Integrins. Cell Tissue Res.
3 Makrilia N., Kollias A., Manolopoulos L., Syrigos K. (2009). Cell adhesion molecules: role and clinical significance in cancer. Cancer Invest.
4 Brooks S.A., Lomax-Browne H.J., Carter T.M., Kinch C.E., Hall D.M. (2010). Molecular interactions in cancer cell metastasis. Acta Histochem.
5 Heino J. (2000). The collagen receptor integrins have distinct ligand recognition and signaling functions. Matrix Biol.
6 Barbolina M.V., Moss N.M., Westfall S.D., Liu Y., Burkhalter R.J., Marga F., Forgacs G., Hudson L.G., Stack M.S. (2009). Microenvironmental regulation of ovarian cancer metastasis. Cancer Treat Res.
7 Kirkland S.C., Ying H. (2008). Alpha2beta1 integrin regulates lineage commitment in multipotent human colorectal cancer cells. J Biol Chem.
8 Hall C.L., Dai J., van Golen K.L., Keller E.T., Long M.W. (2006). Type I collagen receptor (alpha 2 beta 1) signaling promotes the growth of human prostate cancer cells within the bone. Cancer Res.
9 Kiefer J.A., Farach-Carson M.C. (2001). Type I collagen-mediated proliferation of PC3 prostate carcinoma cell line: implications for enhanced growth in the bone microenvironment. Matrix Biol.
10 Staatz W.D., Fok K.F., Zutter M.M., Adams S.P., Rodriguez B.A., Santoro S.A. (1991). Identification of a tetrapeptide recognition sequence for the alpha 2 beta 1 integrin in collagen. J Biol Chem.
11 Huang C.W., Li Z., Cai H., Shahinian T., Conti P.S. (2011). Novel alpha(2)beta(1) integrin-targeted peptide probes for prostate cancer imaging. Mol Imaging.
12 Huang C.W., Li Z., Cai H., Chen K., Shahinian T., Conti P.S. (2011). Design, synthesis and validation of integrin alpha2beta1-targeted probe for microPET imaging of prostate cancer. Eur J Nucl Med Mol Imaging.
13 Huang C.W., Li Z., Cai H., Shahinian T., Conti P.S. (2011). Biological stability evaluation of the alpha2beta1 receptor imaging agents: diamsar and DOTA conjugated DGEA peptide. Bioconjug Chem.
14 Futaki S., Suzuki T., Ohashi W., Yagami T., Tanaka S., Ueda K., Sugiura Y. (2001). Arginine-rich peptides. An abundant source of membrane-permeable peptides having potential as carriers for intracellular protein delivery. J Biol Chem.
15 Arano Y. (1998). Strategies to reduce renal radioactivity levels of antibody fragments. Q J Nucl Med.
16 Huang C.W., Li Z., Conti P.S. (2011). In Vivo Near-Infrared Fluorescence Imaging of Integrin alpha2beta1 in Prostate Cancer with Cell-Penetrating-Peptide-Conjugated DGEA Probe. J Nucl Med.